# Octreotide conjugated to pegylated ultrasmall superparamagnetic iron oxide nanoparticle

Chemical name: | Octreotide conjugated to pegylated ultrasmall superparamagnetic iron oxide nanoparticle
Abbreviated name: | USPIO-PEG-OCT
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptors (SSTRs)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T_2_ primarily and lead to decreased signal. On the other hand, the paramagnetic T_1_ agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T_1_ relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (2). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms (SRIF-14 and SRIF-28) of 14 and 28 amino acids. SST has a short plasma half-life of <3 min (3). Critical to these actions is the expression of SS receptors (SSTRs) present on cells. SSTRs (G-protein coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_-sst_5_) have been identified and subsequently cloned from animal and human tissues (4, 5). ^111^In-DTPA-octreotide (^111^In-DTPA-OC) is a SSTR analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with Single-photon emission computed tomography (6). It has also showed promising results in peptide-receptor radionuclide therapy (7). ^111^In-DTPA-OC binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree but does not bind to sst_1_ and sst_4_ (8). USPIO is composed of iron nanoparticles of 4–6 nm diameters and the hydrodynamic diameter with polyethylene glycol (PEG) coating is 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life of plasma relaxation times is calculated at ~24 h in humans (9) and 2 h in mice (10). Because of its long blood half-life, USPIO can be used as blood pool agent during the early phase of intravenous administration (11). In the late phase, USPIO is suitable for the evaluation of RES in the body, particularly in lymph nodes (12). Li et al. (13) conjugated OCT to USPIO-PEG to form USPIO-PEG-OCT for MRI of SSTRs in tumor.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Somatostatin+receptor%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (Somatostatin receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=somatostatin+receptors%5BAll+Fields%5D+AND+(%22Homo+sapiens%22%5BOrganism%5D+OR+human%5BAll+Fields%5D)), Somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Somatostatin%5BAll+Fields%5D+AND+receptor%5BAll+Fields%5D)
- Clinical trials (Somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))
- Drug information in FDA (Somatostatin receptor (http://google2.fda.gov/search?q=somatostatin+receptor&spell=1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&access=p))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20synthesis)]

A solution of OCT (0.8 mg) was added to a mixture of N-(3-dimethylaminopropyl)-N’-ethylcarbodiimide hydrochloride (5 µmol), N-hydroxysulfosuccinimide (12.5 µmol) and USPIO-PEG nanoparticles (0.8 mg) (13). The pH of the solution was adjusted to 7.5 using NaOH. USPIO-PEG-OCT had a hydrodynamic size of 20 nm. The number of Oct peptides per USPIO-PEG was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20in%20vitro)]

Li et al. (13) performed in vitro uptake studies of USPIO-PEG-OCT and USPIO-PEG (10 µg Fe/ml) in cultured human breast adenocarcinoma MCF-7 cells, which was shown to express SSTRs. A strong uptake of USPIO-PEG-OCT was observed at 12 h after incubation as measured with histological staining of Fe, whereas there was not uptake for USPIO-PEG. Excess OCT was able to block the uptake of USPIO-PEG-OCT. T2-weighted imaging showed that the T2 values of the cells (n = 6/group) incubated with USPIO-PEG-OCT, USPIO-PEG, and buffer were 56.6 ± 13.1, 75.4 ± 16.2, and 86.0 ± 22.4 s, respectively. USPIO-PEG-OCT exhibited a higher negative enhancement of USPIO-PEG-OCT than USPIO-PEG on MCF cells. There were statistically significant differences (P < 0.05) between USPIO-PEG-OCT and USPIO-PEG, and between USPIO-PEG-OCT and buffer. USPIO-PEG-OCT had no effect on the viability of MCF-7 cells in culture up to 80 µg Fe/ml at 12 h of incubation and 20 µg Fe/ml up to 96 h of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20rodentia)]

USPIO-PEG-OCT or USPIO-PEG (7.7 mg Fe/kg) were injected intravenously in the mice bearing MCF-7 tumors (n = 12 mice/group) (13). T2-weighted MR images (3 T) of the tumors were obtained at 0-24 h after injection. There was a loss of signal intensity of 24.49% and 19.81% for USPIO-PEG-OCT and USPIO-PEG at 6 h after injection (P < 0.05), respectively. Both nanoparticles exhibited little loss of signal by 24 h after injection. Histological staining of Fe in tumors showed that there was a large amount of Fe in the tumor tissues of USPIO-PEG-OCT treated mice but not in the tumor tissues of USPIO-PEG treated mice at 6 h after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20octreotide%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
3 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
4 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
5 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
10 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
11 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
12 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
13 Li X., Du X., Huo T., Liu X., Zhang S., Yuan F. (2009). Specific targeting of breast tumor by octreotide-conjugated ultrasmall superparamagnetic iron oxide particles using a clinical 3.0-Tesla magnetic resonance scanner. Acta Radiol.